# N-Benzyl-N-methyl-2-[7,8-dihydro-7-(2-[^18^F]fluoroethyl)-8-oxo-2-phenyl-9H-purin-9-yl]acetamide

Chemical name: | N-Benzyl-N-methyl-2-[7,8-dihydro-7-(2-[^18^F]fluoroethyl)-8-oxo-2-phenyl-9H-purin-9-yl]acetamide
Abbreviated name: | [^18^F]FEDAC
Synonym:
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%5BAll%20Fields%5D)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as central benzodiazepine receptors (CBR) and peripheral benzodiazepine receptors (PBR). PBR is also known as translocator protein (TSPO). The CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBR than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo with positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR antagonistic activity (8). [^11^C]PK11195 has been developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBRs in the central nervous system (9, 10). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than did PK11195 (9, 10). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and [^11^C]DAA1106 have been developed as potential PET ligands with highly selective and specific binding to PBR (11, 12). N-Benzyl-N-methyl-2-[7,8-dihydro-7-(2-[^18^F]fluoroethyl)-8-oxo-2-phenyl-9H-purin-9-yl]acetamide ([^18^F]FEDAC), which has an acetamide structure, has been evaluated for imaging PBR in the brain (13).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610)
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20synthesis)]

Yanamoto et al. (13) reported the synthesis of [^18^F]FEDAC by alkylation of the precursor with [^18^F]FCH_2_CH_2_Br. [^18^F]FEAC was purified with high-performance liquid chromatography with 35% radiochemical yield (decay-corrected) based on [^18^F]F^-^. The total synthesis time was ~45 min. The radiochemical purity was >98% with the specific activity of 30–95 GBq/μmol (0.81–2.43 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20in%20vitro)]

In vitro [^11^C]PK11195 PBR-binding studies using rat brain homogenates showed inhibition constant (K_i_) values of 1.34 ± 0.15 nM and 0.31 ± 0.03 nM for FEDAC and PK11195, respectively (13). Log D was determined to be 3.2 and 3.7 for FEDAC and PK11195, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20rodentia)]

Yui et al. (14) showed that [^18^F]FEDAC had high accumulation as expressed in % injected dose/gram (ID/g) in the lung (27.5), heart (8.3), kidney (15.5), liver (10.3) and small intestine (5.6) in normal mice at 5 min after injection. The brain exhibited 1% ID/g at 1 min and ~0.2% at 90 min. The radioactivity in the bone was 1.9% ID/g at 1 min and 1.3% ID/g at 90 min. PET imaging was performed in rats with infarcted brain. Maximum uptake (1-3 min after injection) on the ipsilateral and contralateral sides was about 0.91 and 0.57 standardized uptake value (SUV), respectively. The SUV ratio of radioactivity between ipsilateral and contralateral sides reached 2.76 for [^18^F]FEDAC at 20 min after injection. The UUV ratio was reduced to ~1 with PK11195 pretreatment (~1 min). The binding potential was estimated to be 1.37 ± 0.06 (n = 4).

Yanamoto et al. (13) performed PET imaging in rats (n = 4) with acute neuroinflammation in the striatum. PET imaging showed an increased accumulation of [^18^F]FEDAC in the lesion as compared with the contralateral side as early as 1 min after injection with rapid clearance. The maximum lesion/normal ratio of 3.0 was achieved within 10–20 min after injection. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20%28primate%20not%20human%29)]

PET imaging was performed in a male rhesus monkey (14). The maximum uptake (0.02% dose/mL) of [18F]FEDAC in the occipital cortex was at ~5 min after injection. At 90 min after injection, the radioactivity decreased to 61% of the maximum.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20human)]

No publications are currently available.

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Gerhard A., Neumaier B., Elitok E., Glatting G., Ries V., Tomczak R., Ludolph A.C., Reske S.N. (2000). In vivo imaging of activated microglia using [11C]PK11195 and positron emission tomography in patients after ischemic stroke. Neuroreport.
9 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
10 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
11 Fujimura Y., Ikoma Y., Yasuno F., Suhara T., Ota M., Matsumoto R., Nozaki S., Takano A., Kosaka J., Zhang M.R., Nakao R., Suzuki K., Kato N., Ito H. (2006). Quantitative analyses of 18F-FEDAA1106 binding to peripheral benzodiazepine receptors in living human brain. J Nucl Med.
12 Maeda J., Suhara T., Zhang M.R., Okauchi T., Yasuno F., Ikoma Y., Inaji M., Nagai Y., Takano A., Obayashi S., Suzuki K. (2004). Novel peripheral benzodiazepine receptor ligand [11C]DAA1106 for PET: an imaging tool for glial cells in the brain. Synapse.
13 Yanamoto K., Kumata K., Yamasaki T., Odawara C., Kawamura K., Yui J., Hatori A., Suzuki K., Zhang M.R. (2009). [18F]FEAC and [18F]FEDAC: Two novel positron emission tomography ligands for peripheral-type benzodiazepine receptor in the brain. Bioorg Med Chem Lett.
14 Yui, J., J. Maeda, K. Kumata, K. Kawamura, K. Yanamoto, A. Hatori, T. Yamasaki, N. Nengaki, M. Higuchi, and M.R. Zhang, 18F-FEAC and 18F-FEDAC: PET of the Monkey Brain and Imaging of Translocator Protein (18 kDa) in the Infarcted Rat Brain. J Nucl Med, 2010